# ^99m^Tc-Labeled cysteine-tagged epidermal growth factor

Chemical name: | ^99m^Tc-Labeled cysteine-tagged epidermal growth factor
Abbreviated name: | [^99m^Tc]Cys-EGF
Synonym:
Agent Category: | Ligand
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the protein and nucleotide sequence (http://www.ncbi.nlm.nih.gov/nuccore/166362727?report=genbank) of human epidermal growth factor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=role+of+growth+factors+in+cancer)]

Growth factors such as the epidermal growth factor (EGF), the vascular endothelial growth factor (VEGF), and the tumor necrosis factor are known to have important roles in the development and progression of cancers (1-3). The EGF mediates its activity through a group of tyrosine kinase (TK)–dependent EGF receptors (EGFR) that promote not only cell proliferation but also cell survival and the motility phenotype that is necessary for the development of an invasive cancer (4). As a consequence, the EGFRs and their associated TKs are the targets of several anti-EGFR antibodies (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+antibodies) and TK inhibitors (http://clinicaltrials.gov/ct2/results?term=EGFR+tyrosine+kinase+inhibitors) that are either approved by the United States Food and Drug Administration or are being evaluated in clinical trials for the treatment of various neoplasms. Before treatment, the patients are screened to determine the extent of EGFR expression in the tumors with the use of immunohistochemistry (IHC) or fluorescence in situ hybridization (FISH) because these techniques help predict the probable therapeutic response and outcome for the individual (5, 6). However, only 10–25% of the patients who are EGFR-positive according to IHC or FISH analysis respond to the anti-EGFR therapy, which indicates that a poor correlation exists between the EGFR expression analysis and the treatment (7, 8). This is probably because only the active receptors are important to predict the efficacy of the anti-EGFR agents for the treatment of cancers, and ICH and FISH do not distinguish between the active and inactive EGFRs (9).

On binding the ligand, a characteristic feature of a functional EGFR is that it is internalized by the cell. Levashova et al. (10) envisioned that perhaps the natural ligand EGF itself could be used as an imaging agent to detect the active EGFRs in tumors. The investigators used an Escherichia coli (E. coli)–expressed EGF containing an N-terminal cysteine fusion tag (Cys-EGF) of 15 amino acids that can be used to conjugate therapeutic or imaging probes as done earlier with VEGF (11). In addition, because an active EGF/EGFR complex is composed of two molecules each of EGF and EGFR, the investigators also bioengineered an N-terminal cysteine fusion tag containing a dimeric EGF (dEGF) molecule in which the second EGF molecule was linked to the first through a linker of 9 amino acids (11). The EGF and the dEGF were then respectively labeled with radioactive technetium (^99m^Tc) to obtain [^99m^Tc]Cys-EGF and [^99m^Tc]Cys-dEGF, which were used to investigate the biodistribution and imaging characteristics of the two molecules in xenograft tumor-bearing mice. It is pertinent to mention here that imaging studies and the biodistribution of only [^99m^Tc]Cys-EGF are described in this chapter. Studies performed with [^99m^Tc]Cys-dEGF are described separately in MICAD (www.micad.nih.gov).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cys-tagged+EGF+synthesis)]

The Cys-EGF was expressed in and purified from E. coli as described elsewhere to obtain Cys-tagged single-chain VEGF (Cys-scVEGF) (12). To label purified Cys-EGF with ^99m^Tc, the protein was first incubated with an equimolar amount of dithiothreitol for 20 min at 25°C in 0.1 M Tris-HCl buffer (pH 8.0) to reduce all the sulfhydryl groups in the tagged protein (11, 12). The reduced protein was then labeled with ^99m^Tc as detailed for Cys-scVEGF (11). The radiolabeled protein (EGF/Tc) was purified with size-exclusion chromatography using a PD-10 column, and the average yield of the labeled product was 45 ± 13% (n = 13 labeling reactions) as determined by the amount of ^99m^Tc eluting from the column (10). The radiochemical purity of EGF/Tc was 90–95% as determined with instant thin-layer chromatography (ITLC) (10). The Rf value for the labeled protein on ITLC was not reported. Specific activity of EGF/Tc was reported to be 5.92–11.10 MBq/mg (0.16–0.30 mCi/mg) (10).

To investigate the stability of EGF/Tc, the labeled protein was injected into mice (n = 2 animals), and then the animals were euthanized 2 min later (10). Blood from the mice was collected and centrifuged to obtain plasma. The plasma was then incubated for 10, 20, and 75 min at 37°C, and the protein-bound radioactivity was determined with ITLC. The radioactivity was reported to be associated with the plasma protein fraction for at least 75 min under these conditions. EGF/Tc was reported to be stable in phosphate-buffered saline for up to 3 h at room temperature as determined by ITLC and denaturing polyacrylamide gel electrophoresis analysis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Cys-EGF+in+vitro)]

Using F98/EGFR(F) rat glioma cells that overexpress the human EGFR, the receptor affinity constant for EGF/Tc was determined with Scatchard’s analysis to be 2.7 nM (10). In another study, Cys-EGF was reported to induce EGFR TK phosphorylation in a dose-dependent manner (10). Cys-EGF was also reported to compete with an EGF-Shiga-like toxin subunit A conjugate (EGF-SLT (http://www.sibtech.com/?p=targeted_toxins)) for binding to the EGFR (10). EGF-SLT is extremely toxic to MDA23 1luc human breast cancer cells that express the EGFR, and the ability of proteins to compete for binding with the EGFR was measured by counting the number of cells surviving after a 72-h exposure to EGF-SLT. The MDA23 1luc cells were exposed to EGF-SLT in the presence of an increasing concentration of Cys-EGF for 72 h. It was reported that cell survival increased with an increasing Cys-EGF concentration, which indicates that Cys-EGF protected the cells from EGF-SLT toxicity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+rodentia)]

Levashova et al. studied the blood clearance and biodistribution of EGF/Tc in mice (n = 4 animals) bearing MDA23 1luc cell tumors (10). The animals were injected with the radiotracer, and blood was collected at preselected time points for up to 60 min. More than 95% of the radioactivity was reported to clear from blood within 60 min. To determine biodistribution of the labeled protein, the animals were euthanized 3 h after administration of the tracer, all the major organs and tumors were harvested, and the incorporated radioactivity was counted in a gamma counter. The radioactivity was reported to have accumulated primarily in the liver (14.6 ± 2.3% injected dose/gram tissue (% ID/g)) and kidneys (27.0 ± 4.8% ID/g). Also, the outer edges and the center of each tumor were reported to have a similar accumulation of radioactivity, indicating that the tracer was distributed throughout the tumor mass. No blocking studies were reported.

The accumulation of EGF/Tc was investigated in mice bearing either orthotopic MDA23 1luc cell tumors or spontaneous lung carcinoma (10). The animals (n = 4 mice per model) were injected with the radiolabeled protein and imaged 1 h later with single-photon emission computed tomography (SPECT). Compared with the surrounding normal tissue, accumulation of radioactivity in the tumors was reported to be clearly evident with both tumor types.

Autoradiography of cryosections prepared from the MDA23 1luc tumors (n = 2 animals) immediately after SPECT imaging confirmed that accumulated radioactivity after EGF/Tc treatment was significantly higher in the tumors than in the normal muscle tissue.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Wu W.K., Tse T.T., Sung J.J., Li Z.J., Yu L., Cho C.H. (2009). Expression of ErbB receptors and their cognate ligands in gastric and colon cancer cell lines. Anticancer Res.
2 Schoenleber S.J., Kurtz D.M., Talwalkar J.A., Roberts L.R., Gores G.J. (2009). Prognostic role of vascular endothelial growth factor in hepatocellular carcinoma: systematic review and meta-analysis. Br J Cancer.
3 Balkwill F. (2009). Tumour necrosis factor and cancer. Nat Rev Cancer.
4 Wilkins-Port C.E., Ye Q., Mazurkiewicz J.E., Higgins P.J. (2009). TGF-beta1 + EGF-initiated invasive potential in transformed human keratinocytes is coupled to a plasmin/MMP-10/MMP-1-dependent collagen remodeling axis: role for PAI-1. Cancer Res.
5 Baselga J., Arteaga C.L. (2005). Critical update and emerging trends in epidermal growth factor receptor targeting in cancer. J Clin Oncol.
6 Varella-Garcia M., Mitsudomi T., Yatabe Y., Kosaka T., Nakajima E., Xavier A.C., Skokan M., Zeng C., Franklin W.A., Bunn P.A., Hirsch F.R. (2009). EGFR and HER2 genomic gain in recurrent non-small cell lung cancer after surgery: impact on outcome to treatment with gefitinib and association with EGFR and KRAS mutations in a Japanese cohort. J Thorac Oncol.
7 Chung K.Y., Shia J., Kemeny N.E., Shah M., Schwartz G.K., Tse A., Hamilton A., Pan D., Schrag D., Schwartz L., Klimstra D.S., Fridman D., Kelsen D.P., Saltz L.B. (2005). Cetuximab shows activity in colorectal cancer patients with tumors that do not express the epidermal growth factor receptor by immunohistochemistry. J Clin Oncol.
8 Bell D.W., Lynch T.J., Haserlat S.M., Harris P.L., Okimoto R.A., Brannigan B.W., Sgroi D.C., Muir B., Riemenschneider M.J., Iacona R.B., Krebs A.D., Johnson D.H., Giaccone G., Herbst R.S., Manegold C., Fukuoka M., Kris M.G., Baselga J., Ochs J.S., Haber D.A. (2005). Epidermal growth factor receptor mutations and gene amplification in non-small-cell lung cancer: molecular analysis of the IDEAL/INTACT gefitinib trials. J Clin Oncol.
9 Johns T.G., Perera R.M., Vernes S.C., Vitali A.A., Cao D.X., Cavenee W.K., Scott A.M., Furnari F.B. (2007). The efficacy of epidermal growth factor receptor-specific antibodies against glioma xenografts is influenced by receptor levels, activation status, and heterodimerization. Clin Cancer Res.
10 Levashova Z., Backer M.V., Horng G., Felsher D., Backer J.M., Blankenberg F.G. (2009). SPECT and PET imaging of EGF receptors with site-specifically labeled EGF and dimeric EGF. Bioconjug Chem.
11 Levashova Z., Backer M., Backer J.M., Blankenberg F.G. (2008). Direct site-specific labeling of the Cys-tag moiety in scVEGF with technetium 99m. Bioconjug Chem.
12 Backer M.V., Levashova Z., Patel V., Jehning B.T., Claffey K., Blankenberg F.G., Backer J.M. (2007). Molecular imaging of VEGF receptors in angiogenic vasculature with single-chain VEGF-based probes. Nat Med.